# D-Cys-D-Asp-Gly-HCit-Gly-Pro-Gln-D-Cys-Ebes-Lys-polyethylene glycol-cholic acids-Cy5.5 telodendrimer nanoparticles

Chemical name: | D-Cys-D-Asp-Gly-HCit-Gly-Pro-Gln-D-Cys-Ebes-Lys-polyethylene glycol-cholic acids-Cy5.5 telodendrimer nanoparticles
Abbreviated name: | OA02-PEG^5k^-CA_8-_Cy5.5 NPs
Synonym:
Agent category: | Peptide
Target: | Integrin α_3_
Target category: | Receptor
Method of detection: | Optical, Near-Infrared
Source of signal: | Cy5.5
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=152013007), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=152013006) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?db=gene&cmd=Retrieve&dopt=full_report&list_uids=3675) for more information about integrin α_3_β_1_.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=OA02)]

Integrins are a family of cell-surface heterodimeric glycoproteins that mediate diverse biological events involving cell–cell and cell–matrix interactions (1). They consist of an α and a β subunit. They are important for cell adhesion and signal transduction. The α_3_β_1_ integrin plays an important role in normal lung, kidney, cerebral cortical, and epithelial development (2). On the other hand, it affects tumor growth, tumor invasiveness, and metastasis as the α_3_β_1_ integrin is strongly expressed on tumor cells (3, 4). D-Cys-D-Asp-Gly-HCit-Gly-Pro-Gln-D-Cys (OA02) was identified to bind to the α_3_ integrin on human ovarian cancer cells using one-bead-one-compound combinatorial libraries (5, 6). OA02 was conjugated with Cy5.5 to study in vivo biodistribution of the tracer in tumor-bearing mice (7). Cy5.5 is a NIR fluorescent dye with an absorbance maximum at 675 nm and emission maximum at 694 nm with a high extinction coefficient of 250,000 (mol/L)^-1^cm^-1^. OA02-Cy5.5 was found to have a high specific accumulation in α_3_β_1_-positve ES-2 human ovarian tumor cells in nude mice.

Polymeric micelles compose of a core-shell structure formed by amphiphilic block copolymers (telodendrimers) with nanoparticle sizes of 20-60 nm (8). Ligands and labels can be conjugated to the shell surface and drugs can be encapsulated inside the core of micelles. Xiao et al. (9) conjugated OA02 to micelles comprising linear copolymers of polyethylene glycol (PEG) and cholic acids (CA). Cy5.5 was conjugated to the amino group of the proximal Lys between PEG and cholic acid (CA) to form D-Cys-D-Asp-Gly-HCit-Gly-Pro-Gln-D-Cys-Ebes-Lys- PEG^5k^-CA_8_-Cy5.5 telodendrimer nanoparticles (OA02-PEG^5k^-CA_8-_Cy5.5 NPs) for in vivo near-infrared (NIR) fluorescence imaging of α_3-_expressing SKOV-3 human ovarian tumor xenografts in nude mice.

### Related Resource Links:

- Chapters in MICAD (OA02 (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=OA02+AND+micad%5Bbook%5D))
- Gene information in NCBI (α_3_ integrin (http://www.ncbi.nlm.nih.gov/gene/3675), β_1_ integrin (http://www.ncbi.nlm.nih.gov/gene/3688))
- Articles in Online Mendelian Inheritance in Man (OMIM) (α_3_ integrin (http://www.ncbi.nlm.nih.gov/omim/605025), β_1_ integrin (http://www.ncbi.nlm.nih.gov/omim/135630))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=OA02+and+synthesis)]

Alkyne modified OA02 peptide (D-Cys-D-Asp-Gly-HCit-Gly-Pro-Gln-D-Cys-Ebes-Lys-alkyne) was prepared using solid-phase peptide synthesis and conjugated to the N_3_-PEG^5k^-CA_8_ telodendrimer monomer via Cu-catalyzed cyloaddition to form OA02-PEG^5k^-CA_8_ telodendrimer monomer (9). There was one OA02 peptide per telodendrimer monomer (9.9 kDa) as measured with MALDI-TOF mass spectroscopy. Cy5.5 monofunctional N-hydroxysuccinimide (NHS) ester was used to conjugate OA02-PEG^5k^-CA_8_ telodendrimer monomer. The NHS ester of Cy5.5 reacted with the amino group of the proximal Lys between PEG and CA. PEG^5k^-CA_8_ and OA02-PEG^5k^-CA_8_-Cy5.5 telodendrimer monomers were mixed in chloroform in 1:1 molar ratio. After evaporation of chloroform, the residue film was dissolved in phosphate-buffered saline to form OA02-PEG^5k^-CA_8-_Cy5.5 NPs. Non-targeted PEG^5k^-CA_8-_Cy5.5 NPs were also prepared. The number of Cy5.5 and OA02 molecules per NP was not reported. The particle sizes were 20.5 ± 1.9 nm and 21.0 ± 2.3 for OA02-PEG^5k^-CA_8-_Cy5.5 NPs and PEG^5k^-CA_8-_Cy5.5 NPs, respectively. OA02-PEG^5k^-CA_8-_FITC NPs and PEG^5k^-CA_8-_FITC NPs were prepared similarly for in vitro studies.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=OA02+and+in+vitro)]

Receptor-mediated endocytosis of OA02-PEG^5k^-CA_8-_FITC NPs in SKOV-3 human ovarian tumor cells (α_3_-positive) and K562 human erythroleukemia cells (α_3_-negative) was observed by fluorescence confocal microscopy and flow cytometry (9). The fluorescence staining of OA02-PEG^5k^-CA_8-_FITC NPs (2 µM) was confined to the cell membrane and cytoplasm after 2 h of incubation at 37°C. Free OA02 peptide (200 µM) and excess anti-α_3_ antibody inhibited the uptake of OA02-PEG^5k^-CA_8-_FITC NPs in SKOV-3 cells. On the other hand, K562 cells showed minimal uptake of OA02-PEG^5k^-CA_8-_FITC NPs. Flow cytometry analysis showed that SKOV-3 cells exhibited 5-fold higher uptake of OA02-PEG^5k^-CA_8-_FITC NPs than PEG^5k^-CA_8-_FITC NPs. The uptake was inhibited by >70% with 100-fold excess OA02 peptide. Furthermore, uptake of non-targeted NPs and targeted NPs was low and similar in K562 cells. Both NPs were not cytotoxic to SKOV-3 cells after 2 h of incubation.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=OA02+and+rodentia)]

Whole-body NIR fluorescence imaging studies of OA02-PEG^5k^-CA_8-_Cy5.5 NPs or PEG^5k^-CA_8-_Cy5.5 NPs (0.4 nmol Cy5.5) were evaluated in nude mice (n = 3/group) bearing SKOV-3 subcutaneous xenografts after intravenous injection (9). Both NPs were distributed throughout the body of the mice at 10 min after injection. Tumor accumulation of OA02-PEG^5k^-CA_8-_Cy5.5 NPs was apparent at 2 h with clear visualization at 4 h. Tumor retention remained throughout the 24 h of imaging period. On the other hand, tumor accumulation of PEG^5k^-CA_8-_Cy5.5 NPs was not apparent until 8 h after injection with a decrease of fluorescence intensity by 24 h. Ex vivo biodistribution studies of OA02-PEG^5k^-CA_8-_Cy5.5 NPs and PEG^5k^-CA_8-_Cy5.5 NPs were performed at 24 after injection. The tumor accumulation (mean fluorescence intensity, MFI) of OA02-PEG^5k^-CA_8-_Cy5.5 NPs (4,400 AU) was ~70% higher (P < 0.05) than that of PEG^5k^-CA_8-_Cy5.5 NPs (2,600 AU). The accumulations in the normal organs were similar for both tracers with the highest accumulations in the liver (3,000 AU) and urinary bladder (2,500 AU). The muscle exhibited a low background level with MFI value of 1,000 AU. Histo-immunologic analysis of tumor sections showed that OA02-PEG^5k^-CA_8-_Cy5.5 NPs co-localized with vascular endothelial cells (CD31-positive and α_3_-positive) and SKOV-3 tumor cells (α_3_-positive), whereas PEG^5k^-CA_8-_Cy5.5 NPs remained mainly in the perivascular region. PEG^5k^-CA_8-_Cy5.5 NPs were able to extravasate from the tumor vasculatures to bind to the tumor cells. Blocking studies were not performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=OA02+and+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=OA02+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=OA02+and+human)]

No publication is currently available.

## NIH Support

R01 CA140449, R01 CA115483, R01 EB012569

## References

1 Hynes R.O., Lively J.C., McCarty J.H., Taverna D., Francis S.E., Hodivala-Dilke K., Xiao Q. (2002). The diverse roles of integrins and their ligands in angiogenesis. Cold Spring Harb Symp Quant Biol.
2 Hynes R.O. (2002). Integrins: bidirectional, allosteric signaling machines. Cell.
3 Albelda S.M., Mette S.A., Elder D.E., Stewart R., Damjanovich L., Herlyn M., Buck C.A. (1990). Integrin distribution in malignant melanoma: association of the beta 3 subunit with tumor progression. Cancer Res.
4 Hynes R.O. (2002). A reevaluation of integrins as regulators of angiogenesis. Nat Med.
5 Aina, O.H., R. Liu, J.L. Sutcliffe, J. Marik, C.X. Pan, and K.S. Lam, From Combinatorial Chemistry to Cancer-Targeting Peptides. Mol Pharm, 2007
6 Aina O.H., Marik J., Liu R., Lau D.H., Lam K.S. (2005). Identification of novel targeting peptides for human ovarian cancer cells using "one-bead one-compound" combinatorial libraries. Mol Cancer Ther.
7 Aina O.H., Marik J., Gandour-Edwards R., Lam K.S. (2005). Near-infrared optical imaging of ovarian cancer xenografts with novel alpha 3-integrin binding peptide "OA02". Mol Imaging.
8 Xiao K., Luo J., Fowler W.L., Li Y., Lee J.S., Xing L., Cheng R.H., Wang L., Lam K.S. (2009). A self-assembling nanoparticle for paclitaxel delivery in ovarian cancer. Biomaterials.
9 Xiao K., Li Y., Lee J.S., Gonik A.M., Dong T., Fung G., Sanchez E., Xing L., Cheng H.R., Luo J., Lam K.S. (2012). "OA02" peptide facilitates the precise targeting of paclitaxel-loaded micellar nanoparticles to ovarian cancer in vivo. Cancer Res.